# ^99m^Tc-Interleukin-2

Chemical name: | ^99m^Tc-Interleukin-2
Abbreviated name: | ^99m^Tc-IL-2
Synonym:
Agent Category: | Polypeptide
Target: | IL-2 receptors (IL-2R)
Target Category: | Receptor binding
Method of detection: | SPECT, planar
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=28178861), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_000586.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=3558) for more information about IL-2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2899mTc%20Interleukin-2%29%20or%20%2899mTc-IL-2%29)]

Interleukin-2 (IL-2) is a T-cell growth factor secreted by T lymphocytes (1). It stimulates the growth and differentiation of T cells, B cells, NK cells, LAK cells, monocytes, macrophages, and oligodendrocytes (2-4). Three subunits (α, β, and γ) of the IL-2 receptor (IL-2R) have been identified. The α subunit has low affinity and normally expresses very low levels in resting lymphocytes (5). The high-affinity receptor is expressed mainly on activated T cells and macrophages (6) when the α, β, and γ subunits associate together (7). Activated cells are found in infiltrating tumors, inflammatory tissues, and autoimmune tissues.

[^123^I]IL-2 has been developed as a single-photon emission computed tomography (SPECT) tracer for imaging activated immune cells in tumors and pathological tissues (8-10). However, ^123^I is a cyclotron radionuclide and therefore is expensive and not readily available. On the other hand, the ready availability and low cost of ^99m^Tc led to the development of ^99m^Tc-IL-2 for studying activated cells in tissues and tumors (11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2899mTc%20IL-2%29%20and%20development)]

Chianelli et al. (11) reported a two-step synthesis of ^99m^Tc-IL-2 using the bifunctional chelating agent S-tetrahydrofurfurylacetyl-(thio-2,3,5,6-tetrafluorophenyl)-adipylglycylglycine, a ligand with two active sites: one providing a N,S set of donor atoms for coordination of ^99m^Tc, and the other, a tetrafluorophenyl-active ester, for protein conjugation via the amino groups on lysine residues of IL-2. The N_3_S of the chelating agent (17 μg) was first complexed with 2 GBq (54 mCi) ^99m^Tc-pertechnetate at 80°C for 20 min and then conjugated to IL-2 (100 ug) at room temperature for 45 min. Radiochemical purity was >99% after Sep-Pak purification with a specific activity of 6.2 GBq/μmol (229 mCi/μmol). The conjugation efficiency was 89.3 ± 7.7%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc%20Interleukin-2%29%20or%20%2899mTc-IL-2%29%29%20and%20in%20vitro)]

In a saturation binding experiment, ^99m^Tc-IL-2 exhibited a binding constant (K_d_) of 10 nM in human peripheral blood mononuclear cells (11). The binding of ^99m^Tc-IL-2 (16 nM) to the cells was inhibited progressively by increasing concentration of anti-CD25 (IL-2α receptor) antibody. The binding of FITC-IL-2 to the cells was inhibited similarly by ^99m^Tc-IL-2 and by unlabeled IL-2 using flow cytometric analyses. Therefore, the binding capacity of ^99m^Tc-IL-2 was not altered by the labeling procedures.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc%20Interleukin-2%29%20or%20%2899mTc-IL-2%29%29%20and%20rodentia)]

Chianelli et al. (11) observed no significant accumulation of ^99m^Tc-IL-2 in major organs except in the kidneys and, to a lesser extent, in the liver and spleen in normal mice at 45 min after injection with significant radioactivity in the urinary bladder. There was negligible radioactivity in the lungs and blood. On the other hand, [^125^I]IL-2 showed a higher degree of kidney uptake and a lower degree of liver uptake.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc%20Interleukin-2%29%20or%20%2899mTc-IL-2%29%29%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc%20Interleukin-2%29%20or%20%2899mTc-IL-2%29%29%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc%20Interleukin-2%29%20or%20%2899mTc-IL-2%29%29%20and%20human)]

Annovazzi et al. (12) performed SPECT studies with ^99m^Tc-IL-2 and ^99m^Tc-labeled granulocytes (^99m^Tc-WBC) in 29 patients with inactive Crohn’s disease, showing that 18 patients (62%) had a positive ^99m^Tc-IL-2 scan and 18 (62%) a positive ^99m^Tc-WBC scan. Only 12 patients (41.4% of the total group) were positive on both scans. Both ^99m^Tc-IL-2 and ^99m^Tc-WBC scintigraphy showed a high negative predictive value (1.00 and 0.91, respectively) but a weak positive predictive value (0.44 and 0.39, respectively). However, Kaplan-Meier curves generated between scintigraphic findings and time free from disease relapse were statistically different only for ^99m^Tc-IL-2 scintigraphy (log rank test, P = 0.013).

Signore et al. (13) performed ^99m^Tc-IL-2 scintigraphy in 30 patients with melanoma lesions. There was uptake of ^99m^Tc-IL-2 in 15 of 21 (71%) melanomas and 2 of 9 (22%) benign cutaneous lesions. The tumor/background ratios (1.10–1.81) correlated significantly with the number of IL-2R-positive (CD25-positive) tumor-infiltrating lymphocytes as determined by histological analyses.

Annovazzi et al. (14) studied carotid atherosclerosis imaging with ^99m^Tc-IL-2 scintigraphy in humans. The degree of ^99m^Tc-IL-2 uptake was expressed as the plaque/background (T/B) ratio. In 14 patients (16 plaques), T/B ratios (1.60-3.47) correlated with the percentage of IL-2R-positive cells at histology (r = 0.707; P = 0.002) and the number of IL-2R–positive cells (T lymphocytes, macrophages, endothelial cells, and smooth muscle cells) at flow cytometry (r = 0.711; P = 0.006). No correlations were observed between ultrasound scores and either scintigraphic or histological findings. In another group of 9 patients (13 plaques), 6 patients were randomly assigned to atorvastatin (a lipid-lowering agent, 20 mg/day) treatment protocol and 3 patients completed a standard hypocholesterolemic diet for 3 months. The mean ^99m^Tc-IL-2 uptake decreased in atorvastatin-treated patients (1.75 ± 0.50 versus 2.16 ± 0.44; P = 0.012), whereas uptake was unchanged in the patients on the hypocholesterolemic diet (2.33 ± 0.45 versus 2.34 ± 0.50). However, the diet study may be too short to see effects and there were only 3 patients.

## References

1 Smith K.A. (1984). Interleukin 2. Annu Rev Immunol.
2 Miyajima A., Miyatake S., Schreurs J., De Vries J., Arai N., Yokota T., Arai K. (1988). Coordinate regulation of immune and inflammatory responses by T cell-derived lymphokines. Faseb J.
3 Muraguchi A., Kehrl J.H., Longo D.L., Volkman D.J., Smith K.A., Fauci A.S. (1985). Interleukin 2 receptors on human B cells. Implications for the role of interleukin 2 in human B cell function. J Exp Med.
4 Smith K.A. (1992). Interleukin-2. Curr Opin Immunol.
5 Robb R.J., Munck A., Smith K.A. (1981). T cell growth factor receptors. Quantitation, specificity, and biological relevance. J Exp Med.
6 Smith K.A. (1989). The interleukin 2 receptor. Annu Rev Cell Biol.
7 Signore A., Procaccini E., Annovazzi A., Chianelli M., van der Laken C., Mire-Sluis A. (2000). The developing role of cytokines for imaging inflammation and infection. Cytokine.
8 Signore A., Beverley P.C., Parman A., Negri M., Pozzilli P. (1987). Labelling of interleukin-2 (IL-2) with 123-iodine with retention of its capacity to bind to activated lymphocytes. Exp Clin Endocrinol.
9 Signore A., Chianelli M., Toscano A., Monetini L., Ronga G., Nimmon C.C., Britton K.E., Pozzilli P., Negri M. (1992). A radiopharmaceutical for imaging areas of lymphocytic infiltration: 123I-interleukin-2. Labelling procedure and animal studies. Nucl Med Commun.
10 Signore A., Chianelli M., Annovazzi A., Bonanno E., Spagnoli L.G., Pozzilli P., Pallone F., Biancone L. (2000). 123I-interleukin-2 scintigraphy for in vivo assessment of intestinal mononuclear cell infiltration in Crohn's disease. J Nucl Med.
11 Chianelli M., Signore A., Fritzberg A.R., Mather S.J. (1997). The development of technetium-99m-labelled interleukin-2: a new radiopharmaceutical for the in vivo detection of mononuclear cell infiltrates in immune-mediated diseases. Nucl Med Biol.
12 Annovazzi A., Biancone L., Caviglia R., Chianelli M., Capriotti G., Mather S.J., Caprilli R., Pallone F., Scopinaro F., Signore A. (2003). 99mTc-interleukin-2 and (99m)Tc-HMPAO granulocyte scintigraphy in patients with inactive Crohn's disease. Eur J Nucl Med Mol Imaging.
13 Signore A., Annovazzi A., Barone R., Bonanno E., D'Alessandria C., Chianelli M., Mather S.J., Bottoni U., Panetta C., Innocenzi D., Scopinaro F., Calvieri S. (2004). 99mTc-interleukin-2 scintigraphy as a potential tool for evaluating tumor-infiltrating lymphocytes in melanoma lesions: a validation study. J Nucl Med.
14 Annovazzi A., Bonanno E., Arca M., D'Alessandria C., Marcoccia A., Spagnoli L.G., Violi F., Scopinaro F., De Toma G., Signore A. (2006). 99mTc-interleukin-2 scintigraphy for the in vivo imaging of vulnerable atherosclerotic plaques. Eur J Nucl Med Mol Imaging.